# ^111^In-1,4,7,10-tetraazacyclododecane-1,4,7-tris-acetic acid-10-maleimidoethylacetamide-Affibody Z_HER2:2395_-Cys

Chemical name: | ^111^In-1,4,7,10-tetraazacyclododecane-1,4,7-tris-acetic acid-10-maleimidoethylacetamide-Affibody Z_HER2:2395_-Cys
Abbreviated name: | ^111^In-[MMA-DOTA-Cys^61^]-Z_2395_-C, ^111^In-DOTA-Z_2395_-C
Synonym:
Agent category: | Antibody fragment, Affibody
Target: | Epidermal growth factor (EGF) HER2 receptor
Target category: | Receptor
Method of detection: | Single-photon emission computed tomography (SPECT), gamma planar imaging
Source of signal: | ^111^In
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=54792098), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?val=NM_201282.1) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=Graphics&list_uids=1956) for more information about HER2.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=HER2%202395)]

Epidermal growth factor (EGF) is a cytokine of 53 amino acids (6.2 kDa) and is secreted by ectodermic cells, monocytes, kidneys, and duodenal glands (1). EGF stimulates growth of epidermal and epithelial cells. EGF and at least seven other growth factors and their transmembrane receptor kinases play important roles in cell proliferation, survival, adhesion, migration, and differentiation. The EGF receptor (EGFR) family consists of four transmembrane receptors: EGFR (HER1/erbB-1), HER2 (erbB-2/neu), HER3 (erbB-3), and HER4 (erbB-4) (2). HER1, HER3, and HER4 comprise three major functional domains: an extracellular ligand-binding domain, a hydrophobic transmembrane domain, and a cytoplasmic tyrosine kinase domain. No ligand has been clearly identified for HER2. However, HER2 can be activated as a result of ligand binding to other HER receptors with the formation of receptor homodimers and/or heterodimers (3). HER1 and HER2 are overexpressed on many solid tumor cells such as breast, non-small cell lung, head and neck, and colon cancers (4-6). The high levels of HER1 and HER2 expression on cancer cells are associated with a poor prognosis (7-10).

Trastuzumab is a humanized IgG_1_ monoclonal antibody (mAb) against the extracellular domain of recombinant HER2 with an affinity constant (K_D_) of 0.1 nM (11). ^111^In-Trastuzumab, Cy5.5-trastuzumab, and ^68^Ga-trastuzumab-F(ab')_2_ have been developed for imaging of human breast cancer (12-16). However, the pharmacokinetics of the intact radiolabeled mAb, with high liver uptake and slow blood elimination, are generally not ideal for imaging. Smaller antibody fragments, such as Fab or F(ab´)_2_, have better imaging pharmacokinetics because they are rapidly excreted by the kidneys. A novel class of recombinant affinity ligands (Affibody molecules) for HER2 was constructed on the basis of the Z-domain residues (58 amino acids) from one of the IgG-binding domains of staphylococcal protein A (17). Affibody molecules exhibit high binding affinity to HER2 with K_D_ values <100 pM. Various radiolabeled Affibody molecules have been studied in terms of their ability to image HER2 in tumors [PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=affibody%20and%20HER2)]. A cysteine molecule was introduced at the C-terminus of Affibody molecules for site-specific coupling with the chelator 1,4,7,10-tetraazacyclododecane-1,4,7-tris-acetic acid-10-maleimidoethylacetamide (MMA-DOTA) for ^111^In labeling (^111^In-[MMA-DOTA-Cys^61^]-Z_2395_-C). ^111^In-[MMA-DOTA-Cys^61^]-Z_2395_-C has been evaluated in nude mice bearing human colon adenocarcinoma tumors (18).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=HER2%202395%20and%20synthesis)]

Affibody Z_2395_-C was reduced with dithiothreitol in 0.02 M ascorbic acid for 18 h at 37°C (18). The reduced Z_2395_-C was incubated with MMA-DOTA in 1:1 molar ratio in ammonium acetate buffer (pH 5.5) for 18 h at 37°C. The coupling efficiency was 93% as determined by LC-MS analysis. There was ~1 chelator per antibody. MMA-DOTA-Z_2395_-C was isolated with column chromatography. MMA-DOTA-Z_2395_-C (25 µg) was mixed with 7.5 MBq (0.2 mCi) ^111^InCl_3_ and incubated for 60 min. The labeling efficiency of ^111^In incorporation was >93%. Specific activity of the preparation was 7 GBq/µmol (189 mCi/µmol). ^111^In-[MMA-DOTA-Cys^61^]-Z_2395_-C was found to be stable after incubation for 3 h in the presence of 1,000-fold molar excess of ethylenediaminetetraacetic acid.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=HER2%202395%20and%20in%20vitro)]

Ahlgren et al. (18) performed binding experiments with Z_2395_-C with the use of a Biacore sensor chip immobilized with extracellular domain of HER2 protein. The K_D_ value of Z_2395_-C was calculated to be 27 pM. The K_D_ value of Z_HER2:342_ was 22 pM. Hence, the binding affinity of Z_2395_-C was about the same as the parent Affibody molecule Z_HER2:342_. In vitro binding specificity tests showed that binding of Z_2395_-C to SKOV-3 cells expressing HER2 was receptor-mediated because saturation of receptors by preincubation with non-labeled Z_HER2:342_ significantly decreased binding of ^111^In-[MMA-DOTA-Cys^61^]-Z_2395_-C. The cell-bound radioactivity remained at 79% of the initially bound activity for up to 24 h when the cells were incubated with ^99m^Tc-Z_2395_-C.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=HER2%202395%20and%20rodentia)]

Ahlgren et al. (18) performed ex vivo biodistribution studies of 0.1 MBq (2.7 μCi) ^111^In-[MMA-DOTA-Cys^61^]-Z_2395_-C in nude mice bearing LS174T xenograft tumors. ^99m^Tc-Z_2395_-C (0.14 nmol) was injected intravenously into each mouse. The initial tracer accumulation in the LS174T tumors was 12% injected dose per gram (ID/g) at 1 h and 10% ID/g at 4 h after injection. The radioactivity level in tumors was higher than in other organs and tissues (the lung, liver, spleen, and intestines) except in the kidneys (117–200% ID/g) at these time points. Blood levels were ~0.73% ID/g at 1 h and 0.1% ID/g at 4 h. The biodistribution was characterized by rapid clearance of radioactivity from blood. Tumor/blood ratios were 18 and 116 at 1 and 4 h after injection, respectively. Preadministration of Z_HER2:342_ (600 µg (83 nmol)) decreased tumor accumulation by >95% (P = 0.005) at 4 h after injection.

Single-photon emission computed tomography analysis was performed in nude mice bearing the LS174T tumors after injection of 3 MBq (81 μCi) ^111^In-[MMA-DOTA-Cys^61^]-Z_2395_-C. The tumor was clearly visualized at 1 h along with the kidneys. In mice pretreated with Z_HER2:342_, the tumors were marginally visualized with ^111^In-[MMA-DOTA-Cys^61^]-Z_2395_-C. Tumor/muscle ratios were 11.8 and 2.9 with blocking.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=HER2%202395%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=HER2%202395%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=HER2%202395%20and%20human)]

No publication is currently available.

## References

1 Carpenter G., Cohen S. (1990). Epidermal growth factor. J Biol Chem.
2 Yarden Y. (2001). The EGFR family and its ligands in human cancer: signalling mechanisms and therapeutic opportunities. Eur J Cancer.
3 Rubin I., Yarden Y. (2001). The basic biology of HER2. Ann Oncol.
4 Grunwald V., Hidalgo M. (2003). Developing inhibitors of the epidermal growth factor receptor for cancer treatment. J Natl Cancer Inst.
5 Mendelsohn J. (1990). Anti-epidermal growth factor receptor monoclonal antibodies as potential anti-cancer agents. J Steroid Biochem Mol Biol.
6 Yasui W., Sumiyoshi H., Hata J., Kameda T., Ochiai A., Ito H., Tahara E. (1988). Expression of epidermal growth factor receptor in human gastric and colonic carcinomas. Cancer Res.
7 Ang K.K., Berkey B.A., Tu X., Zhang H.Z., Katz R., Hammond E.H., Fu K.K., Milas L. (2002). Impact of epidermal growth factor receptor expression on survival and pattern of relapse in patients with advanced head and neck carcinoma. Cancer Res.
8 Costa S., Stamm H., Almendral A., Ludwig H., Wyss R., Fabbro D., Ernst A., Takahashi A., Eppenberger U. (1988). Predictive value of EGF receptor in breast cancer. Lancet.
9 Ethier S.P. (1995). Growth factor synthesis and human breast cancer progression. J Natl Cancer Inst.
10 Yarden Y. (2001). Biology of HER2 and its importance in breast cancer. Oncology.
11 Carter P., Presta L., Gorman C.M., Ridgway J.B., Henner D., Wong W.L., Rowland A.M., Kotts C., Carver M.E., Shepard H.M. (1992). Humanization of an anti-p185HER2 antibody for human cancer therapy. Proc Natl Acad Sci U S A.
12 Perik P.J., Lub-De Hooge M.N., Gietema J.A., van der Graaf W.T., de Korte M.A., Jonkman S., Kosterink J.G., van Veldhuisen D.J., Sleijfer D.T., Jager P.L., de Vries E.G. (2006). Indium-111-labeled trastuzumab scintigraphy in patients with human epidermal growth factor receptor 2-positive metastatic breast cancer. J Clin Oncol.
13 Lub-de Hooge M.N., Kosterink J.G., Perik P.J., Nijnuis H., Tran L., Bart J., Suurmeijer A.J., de Jong S., Jager P.L., de Vries E.G. (2004). Preclinical characterisation of 111In-DTPA-trastuzumab. Br J Pharmacol.
14 Garmestani K., Milenic D.E., Plascjak P.S., Brechbiel M.W. (2002). A new and convenient method for purification of 86Y using a Sr(II) selective resin and comparison of biodistribution of 86Y and 111In labeled Herceptin. Nucl Med Biol.
15 Smith-Jones P.M., Solit D., Afroze F., Rosen N., Larson S.M. (2006). Early tumor response to Hsp90 therapy using HER2 PET: comparison with 18F-FDG PET. J Nucl Med.
16 Smith-Jones P.M., Solit D.B., Akhurst T., Afroze F., Rosen N., Larson S.M. (2004). Imaging the pharmacodynamics of HER2 degradation in response to Hsp90 inhibitors. Nat Biotechnol.
17 Wikman M., Steffen A.C., Gunneriusson E., Tolmachev V., Adams G.P., Carlsson J., Stahl S. (2004). Selection and characterization of HER2/neu-binding affibody ligands. Protein Eng Des Sel.
18 Ahlgren S., Orlova A., Rosik D., Sandstrom M., Sjoberg A., Baastrup B., Widmark O., Fant G., Feldwisch J., Tolmachev V. (2008). Evaluation of maleimide derivative of DOTA for site-specific labeling of recombinant affibody molecules. Bioconjug Chem.